# ^11^C-Labeled rhodamine-123

Chemical name: | ^11^C-Labeled rhodamine-123
Abbreviated name: | [^11^C]Rhodamine-123
Synonym:
Agent Category: | Compound
Target: | P-glycoprotein transporter (P-gp)
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of Rhodamine-123 for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rhodamine-123&cmd=DetailsSearch)]

The P-glycoprotein (P-gp; also known as MDR1 or ABCB1) is a member of the ATP-binding cassette transporter family of proteins (the multi-drug resistance (MDR) protein and the breast cancer resistance protein (BCRP) are the other two members of this group of proteins) that is responsible for the rapid transportation of drugs across the cell membrane (uptake and efflux) (1). The structure, functions, and activities of P-gp have been discussed in detail by Giacomini et al. (2) and Sharom (3). Overexpression of these transporters, particularly P-gp, affects the distribution of drugs in various parts of the body, including the central nervous system (CNS), and is responsible for the development of drug resistance in cancer cells (4). In addition, reduced function and expression of P-gp have been suggested to cause slow or reduced clearance of neurotoxic peptides such as the amyloid-β peptide from the neuronal cells, and this has been hypothesized to contribute to the development of Alzheimer’s disease, Parkinson’s disease, or other such neurological conditions (5). There is much interest in studying the role of P-gp at the blood–brain barrier (BBB) with positron emission tomography (PET), using P-gp substrates such as [^11^C]verapamil and [^11^C]desmethyl-loperamide (6). These tracers can measure the decrease in transport function of the P-gp because this decrease results in the accumulation of the label in the brain; however, the uptake of these radiolabeled compounds in normal brain cells as such is very low, and an increase in P-gp function cannot be determined in the tissue with these labeled compounds. Therefore, it was hypothesized that radiolabeled substrates that have a low to moderate affinity for P-gp will probably accumulate in the brain and likely can be used to determine the expression level of this transporter in the tissue or organ (6).

Rhodamine-123 is a fluorescent dye that is used to measure the expression of P-gp in drug-resistant cells, and the National Cancer Institute of the United States uses it to screen for drugs that serve as substrates for MDR1 (6). This fluorescent dye has also been used to investigate the P-gp function in the blood–brain barrier of wild-type (WT) and knockout (KO) mice (mdr 1 a(-/-); these animals lack the P-gp transporter), and the KO rodents were shown to accumulate up to a 4-fold higher amount of rhodamine-123 in the brain compared with the WT animals (6). Similar results were obtained with the WT rodents when they were intravenously infused with rhodamine-123 in the presence of cyclosporine A, an inhibitor of P-gp (6). From these studies, it was concluded that rhodamine-123 was an in vivo substrate for P-gp in mice. The biodistribution of ^131^I-labeled rhodamine-123 has been studied in mice (7). On the basis of information reported in the studies mentioned above, rhodamine-123 was labeled with ^11^C ([^11^C]rhodamine-123; half-life of ^11^C is 20.4 min) and used to study the efflux transporters in WT and various efflux transporter KO mice (organic cation transporter (OCT) 1 and 2 (OCT1/2) KO mice, BCRP KO mice, and MDR-associated protein 1 (MRP1) KO mice; MRP1 is responsible for the cellular efflux of various anti-cancer drugs and contributes to the development of drug resistance) (6). In addition, the biodistribution of [^11^C]rhodamine-123 was investigated with PET in rats and mice (6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5bAll+Fields%5d+AND+micad%5bbook%5d)

Protein (http://www.ncbi.nlm.nih.gov/protein/AAA59575.1) sequence of human P-gp

Information on human P-gp in Gene database (http://www.ncbi.nlm.nih.gov/gene/5243) (Gene ID: 5243)

P-gp in Online Mendelian Inheritance in Man database (OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5bAll+Fields%5d))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=P-glycoprotein&Search=Search) related to P-gp

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b11C%5drhodamine-123%20synthesis&cmd=DetailsSearch)]

The synthesis of [^11^C]rhodamine-123 has been described by Bao et al. (6). The total time required for the synthesis of [^11^C]rhodamine-123 was 35 min. The radiochemical yield, radiochemical purity, and specific activity of the labeled compound (determined at the end of synthesis) were 4.4 ± 1.7%, >95% (as determined with reverse-phase high-performance liquid chromatography (HPLC)), and 13.4 ± 4.4 GBq/μmol (495.8 ± 62.9 mCi/μmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5b11C%5drhodamine-123%20in%20vitro%20studies&cmd=DetailsSearch)]

[^11^C]Rhodamine-123 was reported to have a stability of 99.0 ± 0.9% for at least 1 h in sterile 0.9% sodium chloride at room temperature and for at least 2.5 h in 0.15 M sodium phosphate buffer (pH 7.4) at the same temperature (6). The labeled compound was reported to be stable in rat plasma, whole blood, and forebrain homogenates for at least 2.5 h at 37°C as determined with radio-HPLC (6).

The lipophilicity (LogD_7.4_) of [^11^C]rhodamine-123 was reported to be 0.85 ± 0.01 (n = 6 determinations) as determined with an n-octanol/0.15 M sodium phosphate buffer (pH 7.4) mixture (6).

The plasma-free fractions of [^11^C]rhodamine-123 in mouse and rat blood were determined to be 0.156 ± 0.007 (n = 3 determinations) and 0.09 ± 0.004 (n = 3 determinations), respectively (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5Drhodamine-123%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]rhodamine-123 was investigated with PET in WT mice and WT rats, efflux transporter KO mice, WT rats pretreated with (2R)-anti-5-{3-[4-(10,11-dichloromethanodibenzosuber-5-yl)piperazin-1-yl]-2-hydroxypropoxy}quinolone trihydrochloride (DCPQ; an inhibitor of P-gp; administered intravenously (i.v.) at the rate of 32 mg/kg body weight (BW)) or with cimetidine (an inhibitor of OCT; 30 mg/kg BW i.v.), and in P-gp KO mice pretreated with cimetidine (6). The rats were given 28.9 ± 5.9 MBq (1.07 ± 0.218 mCi) [^11^C]rhodamine-123 through a penile vein catheter, and the mice were injected with 18.1 ± 7.4 MBq (0.67 ± 0.27 mCi) [^11^C]rhodamine-123 through a tail vein catheter as described elsewhere (6). For some studies, the animals were treated with either DCPQ or cimetidine (i.v. administration) at least 30 min before administration of the tracer.

Time-activity curves generated from PET images of rats showed that the uptake of radioactivity in the brain of these animals (n = 3 rats) peaked within 1 min (<0.27 standardized uptake value (SUV)) after the administration of [^11^C]rhodamine-123 (6). A similar trend in tracer accumulation was observed with the mice (n = 3 animals). Rats pretreated with DCPQ (n = 3 animals) showed an ~2-fold increase in the SUV of the brain compared with the untreated animals, suggesting that the P-gp activity in the BBB of the WT rodents did not allow the accumulation of [^11^C]rhodamine-123 in the brain of the WT rats. At the initial time points, the uptake of radioactivity in the hearts of the DCPQ-pretreated rodents was ~5-fold higher than in the brain of the WT animals. Although the label was rapidly lost from the heart, accumulation was observed to remain ~3-fold higher in this organ than in the brain for up to 90 min postinjection (p.i.). The peak SUVs for the liver and kidney of the untreated rats were ~4 and ~8 at 20 min p.i., respectively, and in the DCPQ-treated animals these values increased to ~5 and ~12, respectively. The patterns of radioactivity uptake in the liver and kidney of the WT mice were similar to those of the organs in the WT rats, as described above.

The biodistribution of [^11^C]rhodamine-123 was studied in WT mice (n = 3 animals) and the various efflux transporter KO mice (P-gp KO, OCT1/2 KO, BCRP KO, and MRP1 KO; n = 3–4 rodents/transporter group) as described elsewhere (6). Data obtained from this study were presented as SUV of unchanged [^11^C]rhodamine-123 concentration (Table 1). The amount of unchanged [^11^C]rhodamine-123 present in the plasma and forebrain of the WT and KO mice was relatively low compared with the accumulation in the heart and kidney of the animals. Only the P-gp KO mice showed an increased concentration of the tracer in the forebrain compared with the organs of the WT animals or the other transporter KO rodents. In addition, the tissue/plasma [^11^C]rhodamine-123 concentration ratios (Table 1) for the forebrain, heart, and kidney were relatively higher in the P-gp KO group than in animals from the other groups. These results indicated that the P-gp transporter plays an important role in the uptake and efflux of [^11^C]rhodamine-123 in the various organs of these rodents.

Table 1: Standardized uptake values (SUV) of unchanged [ ^ 11 ^ C]rhodamine-123 in various tissues of WT and efflux transporter KO mice at 30 min p.i ( 6 ).

Tissues | SUV of unchanged [ ^ 11 ^ C]rhodamine-123 concentrations
Tissues | Wild-type | P-gp KO | OCT1/2 KO | BCRP KO | MRP1 KO
Plasma | 0.031 ± 0.032 | 0.008 ± 0.004 | 0.026 ± 0.003 | 0.022 ± 0.008 | 0.014 ± 0.007
Forebrain | 0.071 ± 0.025 (3.0)* | 0.168 ± 0.006 (12.0)* | 0.029 ± 0.011 (0.5)* | 0.031 ± 0.015 (2.0)* | 0.042 ± 0.006 (4.0)*
Heart | 3.40 ± 0.69 (100.0)* | 2.96 ± 0.29 (120.0)* | 3.51 ± 0.41 (100.0)* | 3.13 ± 1.66 (100.0)* | 2.51 ± 0.013 (110.0)*
Kidney | 10.7 ± 2.23 (600.0)* | 12.8 ± 4.9 (>1,000.0)* | 12.7 ± 0.12 (700.0)* | 11.7 ± 3.87 (750.0)* | 12.1 ± 2.35 (>1,100.0)*

*Approximate tissue/plasma ratios of unchanged [ ^ 11 ^ C]rhodamine-123 ( 6 ).

From these studies, the investigators concluded that P-gp and other such transporters play a very important role in the biodistribution of [^11^C]rhodamine-123 in the brain and peripheral organs of the rodents (6). Therefore, [^11^C]rhodamine-123 is not an ideal tracer to measure the level of P-gp activity in the BBB of these animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5Drhodamine-123%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5Drhodamine-123%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5Drhodamine-123%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Supported by the Intramural Research Program, National Institute of Mental Health, National Institutes of Health.

## References

1 Haar C.P., Hebbar P., Wallace G.C.t., Das A., Vandergrift W.A., Smith J.A., Giglio P., Patel S.J., Ray S.K., Banik N.L. (2012). Drug resistance in glioblastoma: a mini review. Neurochem Res.
2 Giacomini K.M., Huang S.M., Tweedie D.J., Benet L.Z., Brouwer K.L., Chu X., Dahlin A., Evers R., Fischer V., Hillgren K.M., Hoffmaster K.A., Ishikawa T., Keppler D., Kim R.B., Lee C.A., Niemi M., Polli J.W., Sugiyama Y., Swaan P.W., Ware J.A., Wright S.H., Yee S.W., Zamek-Gliszczynski M.J., Zhang L. (2010). Membrane transporters in drug development. Nat Rev Drug Discov.
3 Sharom F.J. (2011). The P-glycoprotein multidrug transporter. Essays Biochem.
4 Hitchcock S.A. (2012). Structural modifications that alter the P-glycoprotein efflux properties of compounds. J Med Chem.
5 Bartels A.L. (2011). Blood-brain barrier P-glycoprotein function in neurodegenerative disease. Curr Pharm Des.
6 Bao X., Lu S., Liow J.S., Morse C.L., Anderson K.B., Zoghbi S.S., Innis R.B., Pike V.W. (2012). [(11)C]Rhodamine-123: Synthesis and biodistribution in rodents. Nucl Med Biol.
7 Vora M.M., Dhalla M. (1992). In vivo studies of unlabeled and radioiodinated rhodamine-123. Int J Rad Appl Instrum B.